# ^111^In-p-Benzyl isothiocyanate-1,4,7,10-tetraazacyclododecane-1,4,7,10-tetraacetic acid-14C5 monoclonal antibody

Chemical name: | ^111^In-p-Benzyl isothiocyanate-1,4,7,10-tetraazacyclododecane-1,4,7,10-tetraacetic acid-14C5 monoclonal antibody
Abbreviated name: | ^111^In-p-SCN-Bz-DOTA-14C5
Synonym:
Agent category: | Antibody
Target: | Integrin α_v_β_5_
Target category: | Receptor
Method of detection: | Single-photon emission computed tomography (SPECT), gamma planar
Source of signal: | ^111^In
Activation: | No
Studies: | - In vitro; - Rodents | Structure is currently not available in PubChem (http://pubchem.ncbi.nlm.nih.gov/).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=14C5)]

Extracellular matrix (ECM) adhesion molecules consist of a complex network of fibronectins, collagens, chondroitins, laminins, glycoproteins, heparin sulfate, tenascins, and proteoglycans surrounding connective tissue cells, and they are mainly secreted by fibroblasts, chondroblasts, and osteoblasts (1). Cell substrate adhesion molecules are considered essential regulators of cell migration, differentiation, and tissue integrity. These molecules play a role in inflammation, but they also participate in the process of invasion and metastasis of malignant cells in the host tissue (2). Invasive tumor cells adhere to the ECM components, which provide a matrix environment for their permeation through the basal lamina and underlying interstitial stroma of the connective tissue. Several ECM adhesion molecules and their protein receptors have been studied extensively for their involvement in tumor invasion and metastasis, including the integrins, lectins, selectins, and cadherins (3).

The monoclonal antibody (mAb) 14C5 recognizes an extracellular membrane antigen expressed on SK-BR-3 human breast tumor cells (4, 5). The mAb 14C5 inhibits the adhesion of tumor cells to ECM and tumor growth. The 14C5 antigen is absent on the cell surface of normal tissues and arteries. However, it is present in high amounts on the cell membrane of invasive breast carcinomas and several other malignant tumors (4). Surprisingly, the 14C5 antigen is markedly expressed on the cell surface of fibroblasts surrounding the tumor cells. The 14C5 antigen is determined to have a molecular weight of ~90 kDa, and 14C5 binds the vascular integrin α_v_β_5_ (6). Grzesiak et al. (7) showed that α_v_β_5_ is overexpressed on pancreatic tumor cells (13 of 13 for α_v_ and 10 of 10 for β_5_). ^123/131^I-14C5 has been evaluated as a noninvasive agent for radioimmunodetection and has demonstrated specific accumulation in human lung tumors in nude mice (8). However, iodine-tyrosine–labeled antibodies were catabolized in the lysosomes to generate iodotyrosine, which exits the cell rapidly. Vervoort et al. (9) compared ^123/131^I-14C5, ^111^In-p-benzyl isothiocyanate-1,4,7,10-tetraazacyclododecane-1,4,7,10-tetraacetic acid-14C5 (^111^In-p-SCN-Bz-DOTA-14C5), and ^111^In-p-SCN-Bz-diethylenetriamine pentaacetic acid-14C5 (^111^In-p-SCN-Bz-DTPA-14C5) with ex vivo biodistribution and in vivo single-photon emission computed tomography (SPECT) gamma planar imaging studies in nude mice bearing human pancreatic Capan-1 tumors.

### Related Resource Links:

- Chapters in MICAD (integrin (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=books&Cmd=DetailsSearch&Term=Integrin+AND+micad%5Bbook%5D), 14C5 (http://www.ncbi.nlm.nih.gov/books/?term=14C5+AND+micad%5Bbook%5D))
- Gene information in NCBI (α_v_ integrin (http://www.ncbi.nlm.nih.gov/gene/3685), β_5_ integrin (http://www.ncbi.nlm.nih.gov/gene/3693))
- Articles in Online Mendelian Inheritance in Man (OMIM) (α_v_ integrin (http://www.ncbi.nlm.nih.gov/omim/193210), β_5_ integrin (http://www.ncbi.nlm.nih.gov/omim/147561))
- Clinical trials (integrin (http://www.clinicaltrials.gov/ct2/results?term=RGD))
- Drug information in FDA (integrin (http://google2.fda.gov/search?q=RGD&client=FDAgov&site=FDAgov&lr=&proxystylesheet=FDAgov&output=xml_no_dtd&getfields=*&x=12&y=8))

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=14C5%20and%20synthesis)]

Vervoort et al. (9) performed ^125/131^I-iodination of mAb 14C5 and control mAb002 using Iodogen method as previous described (8). Radiochemical yields were >75% after purification with PD-10 column chromatography. The specific activities of the labeled antibodies were ~5.6 GBq/μmol (151 mCi/μmol), with a radiochemical purity of >98%. p-SCN-Bz-DOTA-14C5 was prepared by conjugation of p-SCN-Bz-DOTA to mAb 14C5 at a molar ratio of 50:1 (pH 9) for 20 h at 4°C. p-SCN-Bz-DPTA-14C5 was prepared by conjugation of p-SCN-Bz-DTPA to 14C5 at a molar ratio of 50:1 (pH 5.5) for 10 min at 25°C. The conjugates were isolated with ultrafiltration. There were 0.6 p-SCN-Bz-DOTA and 1.5 p-SCN-Bz-DPTA moieties per antibody. For ^111^In-labeling, a solution of the conjugates (0.33 nmol) and 3.7 MBq (0.1 mCi) ^111^InCl_3_ in sodium acetate buffer (pH 5.5) was incubated for 60 min at 45°C. ^111^In-p-SCN-Bz-DOTA-14C5 was purified with ultrafiltration, with >60% yield and >98% purity. ^111^In-p-SCN-Bz-DTPA-14C5 was purified with ultrafiltration with >82% yield and >98% purity. The specific activities were estimated to be ~11.2 GBq/nmol (303 mCi/nmol) for ^111^In-14C5 and 5.6 GBq/nmol (152 mCi/nmol) for ^125/131^I-14C5. All radioimmunoconjugates were stable in 50% mouse serum for up to 2 d at 37°C with no loss of immunoreactivity (~78%).

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=14C5%20and%20in%20vitro)]

Vervoort et al. (9) reported that ^125^I-14C5 and ^111^In-p-SCN-Bz-DOTA-14C5 bound to human pancreatic cancer Capan-1 cells with dissociation constant (K_d_) values (n = 3) of 0.11 ± 0.0.1 nM and 0.11 ± 0.0.3 nM, respectively. No specific binding was observed with ^125^I-mAb002. Internalization of ^125^I-14C5 and ^111^In-p-SCN-Bz-DOTA-14C5 into Capan-1 cells was rapid at 37°C. At 24 hours, ^125^I-14C5 exhibited a significantly lower internalized fraction of 6.93 ± 0.88% (n = 6) compared with 49.44 ± 0.75% (n = 3) for ^111^In-p-SCN-Bz-DOTA-14C5 (P < 0.05), and the radioactivity release from these agents in the medium was 64.4% and 19.3%, respectively. The radioactivity of ^111^In-p-SCN-Bz-DOTA-14C5 and ^111^In-p-SCN-Bz-DTPA-14C5 in the medium and cell lysate was primarily present in high molecular-weight form with no free ^111^In, ^111^In-p-SCN-Bz-DOTA or ^111^In-p-SCN-Bz-DTPA (<6%). On the other hand, the radioactivity of ^125^I-14C5 was present in the medium as free ^125^I-iodide or the degraded form with no free ^125^I-iodide in the cell lysate.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=14C5%20and%20rodentia)]

Vervoort et al. (9) performed ex vivo biodistribution studies in nude mice (n = 3/group) bearing Capan-1 tumors at 1, 24, 48, 72, and 168 h after intravenous injection of 0.145 MBq (0.004 mCi) ^111^In-p-SCN-Bz-DOTA-14C5. The tumor accumulation of radioactivity was 2.3, 14.7, 12.9, 14.3, and 9.7% injected dose per gram (ID/g) at 1, 24, 48, 72, and 168 h, respectively. The maximal accumulation for the liver was 13.9% ID/g at 48 h, the kidney was 5.9% ID/g at 24 h, the lung was 5.1% ID/g at 1 h, the spleen was 4.4% ID/g at 1 h, and the pancreas was 0.9% ID/g at 24–72 h. The biexponential blood clearance of ^111^In-p-SCN-Bz-DOTA-14C5 was characterized by a fast distribution phase (half-life (t_1/2,α_) = 24.9 min) and a slow elimination phase (t_1/2,ß_ = 1,166 min). As a comparison using the same tumor model, the tumor accumulation of ^111^In-p-SCN-Bz-DOTA-14C5 was two- to three-fold higher than that of ^111^In-p-SCN-Bz-DPTA-14C5 and ^131^I-14C5 (P < 0.05), whereas radioactivity in the liver, spleen, kidney, lung, and pancreas was similar with the three tracers. No blocking studies were performed.

Planar gamma imaging studies were performed in nude mice bearing Capan-1 tumors at 3, 24, 48, 72, and 96 h after intravenous injection of ^111^In-p-SCN-Bz-DOTA-14C5, ^111^In-p-SCN-Bz-DPTA-14C5, or ^123^I-14C5 (9). Tumors were clearly visualized at 24 h with the three tracers. Tumor radioactivity for ^123^I-14C5 was not detectable at 72 h and 96 h, whereas the tumors were still visualized at 72 h and 96 h for the ^111^In-conjugates. Liver radioactivity of the ^111^In-conjugates was higher than that of ^123^I-14C5. The maximal tumor/background ratios for ^111^In-p-SCN-Bz-DOTA-14C5, ^111^In-p-SCN-Bz-DPTA-14C5, and ^123^I-14C5 were 6.5 at 96 h, 3.8 at 96 h, and 4.1 at 48 h, respectively. No blocking studies were performed.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=radioisotopes%2014C5%20and%20%28dog%20or%20pig%20or%20sheep%20or%20rabbit%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=14C5%20and%20%28primate%20not%20human%29)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=14C5%20and%20human)]

No publication is currently available.

## References

1 Bosman F.T., Stamenkovic I. (2003). Functional structure and composition of the extracellular matrix. J Pathol.
2 Jiang W.G., Puntis M.C., Hallett M.B. (1994). Molecular and cellular basis of cancer invasion and metastasis: implications for treatment. Br J Surg.
3 Albelda S.M. (1993). Role of integrins and other cell adhesion molecules in tumor progression and metastasis. Lab Invest.
4 Coene E., Schelfhout A.M., De Ridder L., De Potter C.R. (1997). Generation of a monoclonal antibody directed against a human cell substrate adhesion molecule and the expression of the antigen in human tissues. Hybridoma.
5 De Potter C.R., Schelfhout A.M., De Smet F.H., Van Damme S., de Ridder L., Dhont E., van Emmelo J. (1994). A monoclonal antibody directed against a human cell membrane antigen prevents cell substrate adhesion and tumor invasion. Am J Pathol.
6 Burvenich I., Schoonooghe S., Vervoort L., Dumolyn C., Coene E., Vanwalleghem L., Van Huysse J., Praet M., Cuvelier C., Mertens N., De Vos F., Slegers G. (2008). Monoclonal antibody 14C5 targets integrin alphavbeta5. Mol Cancer Ther.
7 Grzesiak J.J., Ho J.C., Moossa A.R., Bouvet M. (2007). The integrin-extracellular matrix axis in pancreatic cancer. Pancreas.
8 Lahorte C.M., Bacher K., Burvenich I., Coene E.D., Cuvelier C., De Potter C., Thierens H., Van de Wiele C., Dierckx R.A., Slegers G. (2004). Radiolabeling, biodistribution, and dosimetry of (123)I-mAb 14C5: a new mAb for radioimmunodetection of tumor growth and metastasis in vivo. J Nucl Med.
9 Vervoort L., Burvenich I., Staelens S., Dumolyn C., Waegemans E., Van Steenkiste M., Baird S.K., Scott A.M., De Vos F. (2010). Preclinical evaluation of monoclonal antibody 14C5 for targeting pancreatic cancer. Cancer Biother Radiopharm.